# Gadolinium-diethylenetriaminepentaacetic acid-cyclo(Cys-Asn-Gly-Arg-Cys)-Gly-Lys-quantum dots

Chemical name: | Gadolinium-diethylenetriaminepentaacetic acid-cyclo(Cys-Asn-Gly-Arg-Cys)-Gly-Lys-quantum dots
Abbreviated name: | cNGR-pQDs, Gd-DTPA-cNGR-QDs
Synonym:
Agent category: | Peptide
Target: | Aminopeptidase N (CD13)
Target category: | Enzyme
Method of detection: | Magnetic resonance imaging (MRI); optical, near-infrared (NIR) fluorescence imaging
Source of signal/contrast: | Gadolinium (Gd^3+^), quantum dots (QDs)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Tumor angiogenesis represents a continuous and important process in tumor development in which the tumor attempts to gain an independent blood supply (4). This process is driven by the tumor's overproduction of angiogenic factors, which bind to receptors on nearby vessel endothelial cells. Angiogenesis is essential for the growth of solid tumors and their metastases. Imaging angiogenesis may be useful for monitoring angiogenic treatments of tumors and cardiovascular diseases (5-7). Aminopeptidase N (APN, CD13) is a membrane bound glycoprotein with MMP activity that cleaves unsubstituted, N-terminal amino acids with neutral side chains from peptides (8). APN has been shown to play a role in tumor angiogenesis, invasion, and metastasis (9). In addition to endothelial cells of angiogenic vessels, most cells of myeloid origin, epithelial cells, fibroblasts and smooth muscle cells also express CD13 (10, 11). The tumor homing peptide cyclo(Cys-Asn-Gly-Arg-Cys)-Gly-Lys (cNGR) contains the Asn-Gly-Arg (NGR) motif that binds to APN (12). Gadolinium (Gd^3+^), a lanthanide metal paramagnetic ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination, which lead to brighter contrast images (13, 14). Fluorescent semiconductor quantum dots (QDs) are nanocrystals made of CdSe/CdTe-ZnS with a radius of 1–10 nm (15-17). They can be tuned to emit in a range of wavelengths by changing their sizes and composition, thus providing broad excitation profiles and high absorption coefficients. Oostendorp et al. (18) prepared multimodal cNGR-labeled paramagnetic QDs (cNGR-pQDs) for measurement of tumor angiogenic activity with magnetic resonance imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR+synthesis)]

The cNGR peptide was synthesized using solid-phase peptide synthesis and then labeled on the resin with biotin-succinimidyl ester via the ε-amino group of the lysine (18). cNGR-Biotin was purified with high-pressure liquid chromatography. Streptavidin-QDs (10 streptavidin molecules/QD) were incubated with cNGR-biotin and then with biotinylated poly-lysine dendritic wedge with eight Gd-DTPA moieties in a molar ratio of 1:6:24 at room temperature. Each QD carried a maximum of 192 Gd^3+^ ions and six cNGR peptides.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR+in+vitro)]

The T_1_ relaxivity of cNGR-pQDs was 7.1 ± 0.4 mM^-1^s^-1^ per Gd^3+^ ion at 7 T and 20°C in saline buffer (18).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR+rodentia)]

Oostendorp et al. (18) performed magnetic resonance imaging (7 T) in nude mice (n = 7) bearing human colorectal adenocarcinoma LS174T tumors after intravenous injection of 525 ng cNGR-pQDs or pQDs alone. The changes in R_1_ were spatially heterogeneous and most pronounced at the tumor rim for both cNGR-pQDs and pQDs. The R_1_ changes induced by cNGR-pQDs and pQDs were 0.3 s^-1^ and 0.1 s^-1^, respectively. The two-fold increase in contrast was confirmed by a two-fold better localization of cNGR-pQDs to tumor endothelial cells than pQDs with ex vivo two-photon laser scanning microscopy. The contrast in the tumor rim was ~50-fold greater than in the tumor core or muscle (<0.05 s^-1^). Administration of excess cNGR (0.525 mg/mouse) 10 min after injection of cNGR-pQDs decreased the contrast by ~80% in the tumor rim. Both contrast agents accumulated primarily and similarly in the spleen, heart, liver, and kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR+human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Folkman J. (1995). Angiogenesis in cancer, vascular, rheumatoid and other disease. Nat Med.
5 Sinusas A.J. (2004). Imaging of angiogenesis. J Nucl Cardiol.
6 Carmeliet P. (2004). Manipulating angiogenesis in medicine. J Intern Med.
7 Miller J.C., Pien H.H., Sahani D., Sorensen A.G., Thrall J.H. (2005). Imaging angiogenesis: applications and potential for drug development. J Natl Cancer Inst.
8 Riemann D., Kehlen A., Langner J. (1999). CD13--not just a marker in leukemia typing. Immunol Today.
9 Sato Y. (2004). Role of aminopeptidase in angiogenesis. Biol Pharm Bull.
10 Corti A., Curnis F., Arap W., Pasqualini R. (2008). The neovasculature homing motif NGR: more than meets the eye. Blood.
11 Curnis F., Arrigoni G., Sacchi A., Fischetti L., Arap W., Pasqualini R., Corti A. (2002). Differential binding of drugs containing the NGR motif to CD13 isoforms in tumor vessels, epithelia, and myeloid cells. Cancer Res.
12 Arap W., Pasqualini R., Ruoslahti E. (1998). Cancer treatment by targeted drug delivery to tumor vasculature in a mouse model. Science.
13 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
14 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
15 Zheng G., Li H., Yang K., Blessington D., Licha K., Lund-Katz S., Chance B., Glickson J.D. (2002). Tricarbocyanine cholesteryl laurates labeled LDL: new near infrared fluorescent probes (NIRFs) for monitoring tumors and gene therapy of familial hypercholesterolemia. Bioorg Med Chem Lett.
16 Gao X., Nie S. (2005). Quantum dot-encoded beads. Methods Mol Biol.
17 Pinaud F., Michalet X., Bentolila L.A., Tsay J.M., Doose S., Li J.J., Iyer G., Weiss S. (2006). Advances in fluorescence imaging with quantum dot bio-probes. Biomaterials.
18 Oostendorp M., Douma K., Hackeng T.M., Dirksen A., Post M.J., van Zandvoort M.A., Backes W.H. (2008). Quantitative molecular magnetic resonance imaging of tumor angiogenesis using cNGR-labeled paramagnetic quantum dots. Cancer Res.